# Radioiodinated MLS128 anti-Tn murine monoclonal antibody

Chemical name: | Radioiodinated MLS128 anti-Tn murine monoclonal antibody
Abbreviated name: | Radioiodinated-MLS128
Synonym: | ^125^I/^131^I-MLS128
Agent Category: | Antibody
Target: | Tn antigen
Target Category: | Tumor-associated carbohydrate antigen
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^125^I/^131^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?cmd=PureSearch&db=pubmed&term=%22Tn%20antigen%22)]

Tn antigen is a tumor-associated carbohydrate epitope (N-acetyl-galactosamine (GalNAc)-O-Ser/Thr (GalNAca-O-Ser/Thr)) (1-3). The radioiodinated anti-Tn murine monoclonal antibody (^125^I/^131^I-MLS128 mAb) was developed for in vivo imaging of Tn antigen-expressing tumors (4).

Altered glycosylation on the cell surface is a hallmark of malignant transformation and tumor progression. Incomplete synthesis of the carbohydrate chains and precursor accumulation result in loss of the normal carbohydrate antigens and high expression of the tumor-associated carbohydrate antigens (5-7). Lewis Y, TF, Globo H, GM2, polysialic acid, sialyl Lewis A, Tn, and sialyl Tn are some of the antigens investigated intensively as diagnostic markers or as vaccine antigens (6-9). Tn antigen was first reported as a tumor-associated antigen nearly 40 years ago (10). It is composed of a single GalNAc glycan residue attached via an α-linkage to either the serine (Ser) or the threonine (Thr) of a polypeptide chain (7, 9). In normal tissues, Tn antigen is generally masked by covalently bound terminal carbohydrate moieties, but in tumors it is unmasked because of defective O-glycosylation. Accordingly, Tn antigen is rarely expressed in normal tissues, but it is widely expressed in human carcinomas or hematological cancers. It has been reported that Tn antigen is expressed in 70–90% of breast, colon, lung, bladder, cervical, ovarian, stomach, and prostate tumors (1, 3, 5). The expression levels of the Tn antigen are closely associated with tumor aggressiveness and poor survival of patients (6, 8). In addition, Tn antigen is recognized by the human immune system as a novel epitope, provoking immune responses in patients. There is a strong correlation among the expression of the Tn antigen, the development of the spontaneous antibodies against Tn, and the prognosis of patients with carcinomas. Clinical trials are under way to deliberately provoke or enhance human immune responses by injecting patients with synthetic peptide antigens bearing Tn structure (3, 6, 11-13).

Tn antigen has attracted significant interest as a target for tumor diagnosis and immunotherapy. A number of anti-Tn IgG and IgM mAbs have been generated and investigated for their imaging feasibilities and anti-tumor activities (2, 4, 14-20). The results are generally inconsistent. There are still some issues to be resolved, such as immunogenicity, reduced effectiveness in vivo, and cross-reactivity against type-A blood antigen. Yao et al. developed a radioiodinated anti-Tn MLS128 mAb and tested its feasibility for in vivo imaging of Tn-expressing colorectal tumor xenografts (4).

Note: Investigators from the same research group as Yao et al. also labeled the anti-Tn MLS128 mAb directly with ^111^In (^111^In-MLS128 (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) and investigated its biodistribution and the feasibility of imaging tumors in mice bearing LS180 tumor xenografts. They also tested the imaging feasibilities of two-step targeting with biotinylated MLS128 (Bt-MLS128) and ^125^I-labeled streptavidin (^125^I-SA) (Bt-MLS128-^125^I-SA (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)), and three-step targeting with Bt-MLS128, SA, and ^111^In-biotin (Bt-MLS128-SA-^111^In-biotin (http://www.ncbi.nlm.nih.gov/bookshelf/corehtml/pmc/homepages/bookshelf/micad.html)) in mice with LS180 tumor xenografts (4, 15-18, 21).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

The anti-Tn MLS128 mAb is a mouse IgG3 antibody with κ light chain. It was produced by immunizing mice with LS180 human colorectal cancer cells (19), and the antibody was purified from the ascitic fluid of the hybridoma-bearing mice with protein A affinity chromatography. The antibody was directly radioiodinated using the chloramine-T method (22). The radiolabeled antibody was separated from free iodine through chromatography on PD-10 gel. An isotype-matched control antibody FLOPC21 was also radioiodinated under the same conditions (^125^I-FLOPC21). FLOPC21 is a purified mouse myeloma protein IgG3κ. The specific activity and labeling efficiency values of the radioiodinated antibodies were ~74 MBq/mg (2 mCi/mg) and >99%, respectively. The purity and stability of the radioiodinated antibodies were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Yao et al. analyzed the ability of ^125^I-MLS128 to bind to the LS180 tumor cells in vitro by incubating them together for 1 h at 4ºC (4). The fraction of the immunoreactive antibody was determined with linear extrapolation to conditions representing infinite antigen excess. The affinity constant of the binding was determined using Scatchard plot analysis. The immunoreactive fraction is a parameter used for quality control of antibody radiolabeling (23); it represents how much of the conjugated antibody is able to bind to the relevant antigen. In vitro studies have shown that the immunoreactive fraction and affinity constant of ^125^I-MLS128 were 52.6% and 9.0 × 10^7^ M^-1^, respectively. The binding of ^125^I-MLS128 to the LS180 cells was inhibited by addition of unlabeled MLS128 antibody (data not shown).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22MLS128%22)]

Biodistribution of ^125^I-MLS128 and the control ^125^I-FLOPC21 was studied in female BALB/c nu/nu mice bearing LS180 subcutaneous tumor xenografts (4). Potassium iodide solution was administered to mice 1 day before injection of the antibodies. ^125^I-MLS128 (10 µg, 37 kBq (1 µCi)) was administered via the tail vein. The mice were then euthanized at 6, 24, 48, and 96 h after injection (n = 4 mice/time point), and the radioactivity in each organ was measured. The data showed that ^125^I-MLS128 was well localized the tumors. Accumulation of ^125^I-MLS128 in tumors was rapid and high at 10.61 ± 2.24% injected dose per gram of tissue (ID/g) at 6 h, reaching a peak of 34.69 ± 7.44% ID/g at 48 h after injection. The ratios of tumor/nontumor radioactivity at 48 h reached 4.56, 17.84, and 23.62 for blood, liver, and bone, respectively, and increased thereafter. The biodistribution of the control ^125^I-FLOPC21 in normal organs was similar to that of ^125^I-MLS128, but the tumor uptake of ^125^I-FLOPC21 was very low at only 5.58 ± 0.38% ID/g at 48 h after injection.

To image tumors, 3.7 MBq (0.1 mCi) of ^131^I-MLS128 was administered with 30 µg total antibody dose. The results of scintigraphic imaging were consistent with the biodistribution data. A high tumor uptake was obtained as rapidly as 6 h after injection, and only tumors were discernible after 48 h in the scintigrams of tumor-bearing mice. Yao et al. concluded that the anti-Tn MLS128 mAb is promising for radioimmunoimaging of colorectal cancer (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Springer G.F. (1997). Immunoreactive T and Tn epitopes in cancer diagnosis, prognosis, and immunotherapy. J Mol Med.
2 Ando H., Matsushita T., Wakitani M., Sato T., Kodama-Nishida S., Shibata K., Shitara K., Ohta S. (2008). Mouse-human chimeric anti-Tn IgG1 induced anti-tumor activity against Jurkat cells in vitro and in vivo. Biol Pharm Bull.
3 Li Q., Anver M.R., Butcher D.O., Gildersleeve J.C. (2009). Resolving conflicting data on expression of the Tn antigen and implications for clinical trials with cancer vaccines. Mol Cancer Ther.
4 Yao Z., Sakahara H., Zhang M., Kobayashi H., Nakada H., Yamashina I., Konishi J. (1995). Radioimmunoimaging of colon cancer xenografts with anti-Tn monoclonal antibody. Nucl Med Biol.
5 Babino A., Oppezzo P., Bianco S., Barrios E., Berois N., Navarrete H., Osinaga E. (2000). Tn antigen is a pre-cancerous biomarker in breast tissue and serum in n-nitrosomethylurea-induced rat mammary carcinogenesis. Int J Cancer.
6 Hakomori S. (2001). Tumor-associated carbohydrate antigens defining tumor malignancy: basis for development of anti-cancer vaccines. Adv Exp Med Biol.
7 Kulkarni K.A., Sinha S., Katiyar S., Surolia A., Vijayan M., Suguna K. (2005). Structural basis for the specificity of basic winged bean lectin for the Tn-antigen: a crystallographic, thermodynamic and modelling study. FEBS Lett.
8 Kurtenkov O., Klaamas K., Rittenhouse-Olson K., Vahter L., Sergejev B., Miljukhina L., Shljapnikova L. (2005). IgG immune response to tumor-associated carbohydrate antigens (TF, Tn, alphaGal) in patients with breast cancer: impact of neoadjuvant chemotherapy and relation to the survival. Exp Oncol.
9 Lescar J., Sanchez J.F., Audfray A., Coll J.L., Breton C., Mitchell E.P., Imberty A. (2007). Structural basis for recognition of breast and colon cancer epitopes Tn antigen and Forssman disaccharide by Helix pomatia lectin. Glycobiology.
10 Dausset J., Moullec J., Bernard J. (1959). Acquired hemolytic anemia with polyagglutinability of red blood cells due to a new factor present in normal human serum (Anti-Tn). Blood.
11 Springer G.F., Desai P.R., Spencer B.D., Tegtmeyer H., Carlstedt S.C., Scanlon E.F. (1995). T/Tn antigen vaccine is effective and safe in preventing recurrence of advanced breast carcinoma. Cancer Detect Prev.
12 Slovin S.F., Ragupathi G., Musselli C., Olkiewicz K., Verbel D., Kuduk S.D., Schwarz J.B., Sames D., Danishefsky S., Livingston P.O., Scher H.I. (2003). Fully synthetic carbohydrate-based vaccines in biochemically relapsed prostate cancer: clinical trial results with alpha-N-acetylgalactosamine-O-serine/threonine conjugate vaccine. J Clin Oncol.
13 Cipolla L., Rescigno M., Leone A., Peri F., La Ferla B., Nicotra F. (2002). Novel Tn antigen-containing neoglycopeptides: synthesis and evaluation as anti tumor vaccines. Bioorg Med Chem.
14 Takahashi H.K., Metoki R., Hakomori S. (1988). Immunoglobulin G3 monoclonal antibody directed to Tn antigen (tumor-associated alpha-N-acetylgalactosaminyl epitope) that does not cross-react with blood group A antigen. Cancer Res.
15 Yao Z., Zhang M., Sakahara H., Saga T., Kobayashi H., Nakamoto Y., Toyama S., Konishi J. (1998). Increased streptavidin uptake in tumors pretargeted with biotinylated antibody using a conjugate of streptavidin-fab fragment. Nucl Med Biol.
16 Zhang M., Yao Z., Saga T., Sakahara H., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1998). Improved intratumoral penetration of radiolabeled streptavidin in intraperitoneal tumors pretargeted with biotinylated antibody. J Nucl Med.
17 Zhang M., Yao Z., Sakahara H., Saga T., Nakamoto Y., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Effect of administration route and dose of streptavidin or biotin on the tumor uptake of radioactivity in intraperitoneal tumor with multistep targeting. Nucl Med Biol.
18 Nakamoto Y., Saga T., Sakahara H., Yao Z., Zhang M., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Three-step tumor imaging with biotinylated monoclonal antibody, streptavidin and 111In-DTPA-biotin. Nucl Med Biol.
19 Numata Y., Nakada H., Fukui S., Kitagawa H., Ozaki K., Inoue M., Kawasaki T., Funakoshi I., Yamashina I. (1990). A monoclonal antibody directed to Tn antigen. Biochem Biophys Res Commun.
20 Oppezzo P., Osinaga E., Tello D., Bay S., Cantacuzene D., Irigoin F., Ferreira A., Roseto A., Cayota A., Alzari P., Pritsch O. (2000). Production and functional characterization of two mouse/human chimeric antibodies with specificity for the tumor-associated Tn-antigen. Hybridoma.
21 Zhang M., Sakahara H., Yao Z., Saga T., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1997). Intravenous avidin chase improved localization of radiolabeled streptavidin in intraperitoneal xenograft pretargeted with biotinylated antibody. Nucl Med Biol.
22 Sakahara H., Endo K., Nakashima T., Koizumi M., Kunimatsu M., Kawamura Y., Ohta H., Nakamura T., Tanaka H., Kotoura Y., et al. (1987). Localization of human osteogenic sarcoma xenografts in nude mice by a monoclonal antibody labeled with radioiodine and indium-111. J Nucl Med.
23 Lindmo T., Boven E., Cuttitta F., Fedorko J., Bunn P.A. (1984). Determination of the immunoreactive fraction of radiolabeled monoclonal antibodies by linear extrapolation to binding at infinite antigen excess. J Immunol Methods.